# Quantum dot-A10 RNA aptamer-doxorubicin conjugate

Chemical name: | Quantum dot-A10 RNA aptamer-doxorubicin conjugate
Abbreviated name: | QD-Apt(Dox)
Synonym:
Agent category: | Nucleic acid (nanoparticle)
Target: | Prostate-specific membrane antigen (PSMA)
Target category: | Nucleic acid binding protein
Method of detection: | Optical imaging
Source of signal/contrast: | Quantum dots, doxorubicin
Activation: | No
Studies: | - In vitro | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=QD+Apt+Dox)]

Prostate-specific membrane antigen (PSMA) is a type II membrane glycoprotein with a molecular weight of ~100 kDa (1). PSMA is composed of several domains, including a potential phosphorylation site in the cytoplasmic tail (amino acids 1–18), a highly hydrophobic α-helix in the transmembrane region (amino acids 19–43), and catalytic sites in the extensive extracellular domain (amino acids 44–750). Two unique enzymatic functions are found in PSMA: N-acetylated, α-linked, dipeptidase (NAALADase) activity and folate hydrolase activity. As a prostate cancer cell marker, PSMA expression is primarily prostate-specific, with very low levels (~1,000-fold less) in the brain, salivary glands, and small intestine. PSMA has become an excellent target for imaging and therapy prostate cancer.

Aptamers (from the Latin aptus, to fit, and the Greek meros, part or region) are single-stranded or double-stranded oligonucleotides (RNA or DNA, respectively) that are modified to bind a variety of targets with high binding affinity and specificity (2). Aptamers range in size from 20 to 80 base pairs (~6–26 kDa) with dissociation constants in the range of 10 pM to 10 nM (3). Unlike linear oligonucleotides, which contain genetic information or antisense oligonucleotides that interrupt the transcription of genetic information, aptamers are globular molecules with a shape similar to tRNA and bind to target proteins specifically (4). A10 RNA aptamer (Apt) is a nuclease-stabilized 2’-fluoropyrimidine RNA molecule of 57 base pairs with a molecular weight of 18.5 kDa (5). Its 2’-fluoro-modified ribose on all pyrimidines and 3’-inverted deoxythymidine cap provide significant resistance to nuclease in blood (6). Apt has a single 5’-CG-3’ sequence in its predicted double-stranded stem region, which is a preferred binding site for the anthracycline class of anticancer drugs such as doxorubicin (Dox) (7). Dox intercalates within the GC pair in Apt to form physical conjugate Apt(Dox) at molar ratio of 1.11:1 (dissociation constant = 600 nM) and emit fluorescence simultaneously. Because Dox possesses high efficacy against a range of neoplasms, including acute lymphoblastic and myeloblastic leukemias, malignant lymphomas, soft tissue and bone sarcomas, and breast, ovarian, prostate bladder, gastric, and bronchogenic carcinomas (8), this complex can be used as a PSMA-specific drug carrier to deliver Dox to prostate cancer cells.

Quantum dots (QDs) are semiconductor nanocrystals 2 to 10 nm in diameter (200–10,000 atoms) that possess a quantum confinement effect (hence the name “quantum dots”) caused by the restriction of electrons and holes in all three dimensions (9, 10). Like classic semiconductors that are composed of two types of atoms from the II/VI or III/V group elements in the periodic table, these nanocrystals have a valence band and a conduction band separated by an energy gap (band gap). Upon excitation, an electron is promoted from the filled valence band to the largely empty conduction band, which creates a positive vacancy “hole” in the valence band. The spatial separation (Bohr radius) of this electron-hole pair (“exciton”) is typically 1–10 nm for most semiconductors (10). The quantum confinement arises when one of the dimensions in the nanocrystals becomes comparable to its Bohr radius, at which time these valence/conduction bands are quantized with an energy value that is directly related to the nanocrystal size. Thus, the excitons are confined in a manner similar to a particle-in-the-box problem, leading to a finite band gap and discretization of energy levels. When the electron fills the vacancy in the valence band, light of a certain wavelength is emitted, which corresponds to the respective band gap energy that is a function of nanocrystal size. For instance, the emission wavelength is 550 nm for 3-nm CdSe QDs and 650 nm for 7-nm CdSe QDs (11, 12). For biological applications, QDs are generally encapsulated with biocompatible polymers, functionalized for various bioconjugations, and widely used to label molecules for optical imaging.

The QD-Apt(Dox) conjugate is an PSMA-specific agent used for optical imaging of the delivery of the anticancer drug Dox (13). QD-Apt(Dox) consists of three components: PSMA-specific Apt covalently attached to the core surface as targeting molecule and drug carrier, an anthracycline class of anticancer drug Dox as a therapeutic agent and optical sensor, and a carboxyl core-CdSe/ZnS shell QD (QD490) as a carrier of A10 and Dox and as the second optical sensor. The two sensors (Dox and QD) generate an optical signal via formation of bi-molecular fluorescence resonance energy transfer (Bi-FRET) complex. FRET is a near-field dipole-dipole interaction that involves energy transfer between two molecules in close proximity (3-6 nm). In QD-Apt(Dox), there is a donor-acceptor relationship between QDs and Dox. The fluorescence of both QD and Dox is quenched (“OFF”) when QD-Apt is loaded with Dox, and fluorescence is restored upon the release of Dox (“ON”) after the uptake of QD-Apt(Dox) by prostate cancer cells. Thus, QD-Apt(Dox) can be used to image drug delivery to prostate cancer cells.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( QD+Apt+Dox)+AND+synthesis%0D%0A)]

Bagalkot et al. reported the detailed preparation of QD-Apt(Dox) (13). Initially, commercially available carboxyl core-CdSe/ZnS shell QD was reacted with N-hydroxysuccinimide (NHS) in the presence of 1-ethyl-3-(3-dimethylaminopropyl) carbodiimide (EDC). The produced QD-NHS was then covalently linked to 5’-NH_2_-modified Apt at a molar ratio of 1:10 to yield QD-Apt conjugate. The excess active esterson the QD surface were quenched with ethanolamine 1 h later. Finally, QD-Apt was incubated with Dox to form QD-Apt(Dox).

The mechanism of Dox binding to QD-Apt was examined by fluorescence spectroscopy (13). For a fixed concentration of QD-Apt (10 μM) incubated with an increasing molar ratio of Dox (0 to 8), a sequential decrease in the fluorescence emission spectrum of QD (440–560 nm) was observed when excited at 350 nm. The maximal fluorescence occurred at the molar ratio of 1:7. This result suggested a diminished QD fluorescence caused by an energy transfer from QD to Dox. On the other hand, for a fixed concentration of Dox (10 μM) incubated with an increasing molar ratio of QD-Apt (0 to 0.16), a sequential decrease was also found in the fluorescence emission spectrum of Dox (520–640 nm) when excited at 480 nm, confirming that the quenching of Dox fluorescence was caused by intercalation within Apt on the surface of QDs. These experiments demonstrated that the formation of the QD-Apt(Dox) produced a Bi-FRET system, in which the QD fluorescence was quenched by Dox through a donor-acceptor model between QD and Dox.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( QD+Apt+Dox)+AND+%22in+vitro%22)]

Bagalkot et al. studied the specificity of QD-Apt binding to PSMA with in vitro fluorescent microscopy (13). QD-Apt (100 nM) was incubated with PSMA-expressing prostate cancer cells (LNCaP) and PSMA-negative PC3 cells for 0.5 h at 37ºC. A significant uptake of QD-Apt was found in the LNCaP cells compared with that in the PC3 cells. On the basis of these results, QD-Apt(Dox) was assumed to bind specifically to LNCaP cells. The uptake of QD-Apt(Dox) by LNCaP cells was examined with confocal scanning microscopy as a function of incubation time (13). After incubation for 0.5 h, a faint signal was observed for both internalized QD and Dox (an “OFF” state of Bi-FRET system). At this time, the majority of Dox remained intercalated within the surface Apt, leading to a quenching of both QD and Dox fluorescence. After incubation for 1.5 h, a substantial increase was observed in both QD and Dox fluorescence (an “ON” state of Bi-FRET system). At this time, a substantial amount of Dox was released from the QD-Apt(Dox) caused by either the physical dissociation of Dox from QD-Apt(Dox) or biodegradation of the surface Apt in the lysosomes. Both QD and Dox generated very sharp images of LNCaP cells with low background noise, which allowed in vitro detection of cancer cells at the single-cell level. The cytotoxicity of QD-Apt(Dox) was assessed with an in vitro methylthiazole tetrazolium (MTT) cell proliferation assay (13). LNCaP cells appeared to have lower cellular viability (52.5 ± 1.6%, n = 3) than PC3 cells (77.2 ± 3.1%, n = 3). Because free Dox, QD, and Apt exhibited no apparent cytotoxicity to LNCaP cells or PC3 cells, the higher cytotoxicity of QD-Apt(Dox) found in LNCaP cells might be related to the release of Dox molecules after endocytotic uptake.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( QD+Apt+Dox) +AND++rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( QD+Apt+Dox) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( QD+Apt+Dox) +AND+human)]

No publication is currently available.

### NIH Support

EB 03647, CA119349

## References

1 Ghosh A., Heston W.D. (2004). Tumor target prostate specific membrane antigen (PSMA) and its regulation in prostate cancer. J Cell Biochem.
2 Ng E.W., Shima D.T., Calias P., Cunningham E.T., Guyer D.R., Adamis A.P. (2006). Pegaptanib, a targeted anti-VEGF aptamer for ocular vascular disease. Nat Rev Drug Discov.
3 Levy-Nissenbaum E., Radovic-Moreno A.F., Wang A.Z., Langer R., Farokhzad O.C. (2008). Nanotechnology and aptamers: applications in drug delivery. Trends Biotechnol.
4 Hicke B.J., Stephens A.W. (2000). Escort aptamers: a delivery service for diagnosis and therapy. J Clin Invest.
5 Lupold S.E., Hicke B.J., Lin Y., Coffey D.S. (2002). Identification and characterization of nuclease-stabilized RNA molecules that bind human prostate cancer cells via the prostate-specific membrane antigen. Cancer Res.
6 Farokhzad O.C., Jon S., Khademhosseini A., Tran T.N., Lavan D.A., Langer R. (2004). Nanoparticle-aptamer bioconjugates: a new approach for targeting prostate cancer cells. Cancer Res.
7 Zhang L., Radovic-Moreno A.F., Alexis F., Gu F.X., Basto P.A., Bagalkot V., Jon S., Langer R.S., Farokhzad O.C. (2007). Co-delivery of hydrophobic and hydrophilic drugs from nanoparticle-aptamer bioconjugates. ChemMedChem.
8 Bagalkot V., Farokhzad O.C., Langer R., Jon S. (2006). An aptamer-doxorubicin physical conjugate as a novel targeted drug-delivery platform. Angew Chem Int Ed Engl.
9 Zhang H., Yee D., Wang C. (2008). Quantum dots for cancer diagnosis and therapy: biological and clinical perspectives. Nanomed.
10 Sharma P., Brown S., Walter G., Santra S., Moudgil B. (2006). Nanoparticles for bioimaging. Adv Colloid Interface Sci.
11 Hild W.A., Breunig M., Goepferich A. (2008). Quantum dots - nano-sized probes for the exploration of cellular and intracellular targeting. Eur J Pharm Biopharm.
12 Qi L., Gao X. (2008). Emerging application of quantum dots for drug delivery and therapy. Expert Opin Drug Deliv.
13 Bagalkot V., Zhang L., Levy-Nissenbaum E., Jon S., Kantoff P.W., Langer R., Farokhzad O.C. (2007). Quantum dot-aptamer conjugates for synchronous cancer imaging, therapy, and sensing of drug delivery based on bi-fluorescence resonance energy transfer. Nano Lett.